# ^111^In-Labeled DOTA-conjugated sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], a sulfated cholecystokinin 8 (sCCK8) peptide derivative

Chemical name: | ^111^In-Labeled DOTA-conjugated sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], a sulfated cholecystokinin 8 (sCCK8) peptide derivative
Abbreviated name: | [^111^In]sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^
Synonym:
Agent Category: | Peptide
Target: | Cholecystokinin receptor 2 (CCK2R)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=cck2%20receptor&cmd=DetailsSearch)]

The three subtypes of the cholecystokinin (CCK) receptor (CCKR), designated CCK1R, CCK2R, and CCK2i4svR, belong to the G-protein–coupled receptor family and are classified on the basis of their affinities for the CCK and the gastrin peptides, differential distribution in the tissues, and molecular structure (1). The CCK1R (previously known as CCKA) is found mainly on the peripheral cells of the pancreas and has a 500- to 1,000-fold higher affinity for sulfated CCK8 (sCCK8; contains a sulfated tyrosine (Tyr) residue) compared with the non-sulfated ligand. In addition, CCK1R is expressed mainly in organs of the gastrointestinal tract of rodents, but it is expressed at low levels in humans (2). CCK2R (previously known as CCKB, also designated as the gastrin receptor (GR)) is expressed in the brain, stomach, pancreas, and gallbladder and exhibits an almost equivalent affinity for gastrin and sulfated or non-sulfated CCK. Although CCK1R and CCK2R/GR are expressed in several normal tissues, CCK2R is overexpressed in most cancerous tumors, such as medullary thyroid carcinomas (http://www.cancer.gov/cancertopics/pdq/genetics/medullarythyroid/HealthProfessional) (>90%), astrocytomas (http://www.cancer.gov/dictionary?cdrid=45602) (>65%), and stromal ovarian cancers (http://www.cancer.gov/cancertopics/types/ovarian) (100%). The CCK2i4svR is a splice variant of the CCK2R that is expressed only in colorectal and pancreatic neoplasms and is not detectable in normal colorectal mucosa (1). Several gastrin and CCK8 analogs that have a high affinity for CCK2R have been developed and labeled with radionuclides for the detection and therapy of these cancers. It has been shown that radiolabeled CCK8 derivatives and minigastrin (MG0; a shorter version of human gastrin 1 that consists of amino acids 5–17 of the parent peptide) can be used with scintigraphy to detect colorectal or pancreatic cancer tumors that overexpress CCK2i4svR (3) or to screen for patients who may benefit from the radiotherapy of this disease (4). In preclinical studies, however, a high uptake of radioactivity in the kidneys was observed with these radiochemicals, and it was concluded that these tracers will be of limited use in humans (5). In addition, the sulfated Tyr residue at position 2 in sCCK8 is rapidly hydrolyzed, and the two methionine (Met) residues at positions 3 and 6 in the peptide can be easily oxidized during radiolabeling procedures or under in vivo conditions (6).

Two cyclized MG analogs, cyclo-MG1 and cyclo-MG2, were synthesized, labeled with ^99m^Tc, and evaluated with single-photon emission computed tomography (SPECT) for the detection of tumors that express CCKR (7). Although the two ^99m^Tc-labeled cyclo-compounds were suitable for the detection of tumors, they had low in vitro stability and generated low-quality scintigraphic images because they rapidly degraded under in vivo conditions. Similar observations have been reported with other ^99m^Tc-labeled compounds that were used in clinical trials for the visualization of tumors that overexpressed the CCK2R (8). In an ongoing effort to develop imaging agents that can be used to visualize tumors that express CCK2R, a stabilized sCCK8 derivative was prepared by replacing the sulfated Tyr in the molecule with a sulfated phenylalanine (Phe^2^(p-CH_2_SO_3_H)) and by substituting the Met residues in the peptide with either norleucine (Nle) (sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^]) or homoproparglyglycine (HPG; sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^]) (6). To facilitate the radiolabeling of these compounds with ^111^In, the peptides, including sCCK8 and sCCK8[Phe^2^(p-CH_2_SO_3_H)], were conjugated with 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA). The biodistribution of [^111^In]-DOTA-sCCK8, [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H)], [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] was compared in athymic BALB/c nude mice bearing AR42J (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1492&Template=cellBiology) cell tumors that express CCK2R (6). In another study, the biodistribution of [^111^In/^68^Ga]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] was compared with that of [^111^In/^68^Ga]-DOTA-sCCK8 and [^111^In/^68^Ga]-DOTA-MG0 in athymic BALB/c nude mice bearing tumors generated from A431 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology) cells transfected with CCK2R (9). This chapter describes studies performed only with the ^111^In-labeled peptides. Results obtained with the ^68^Ga-labeled peptides are described in a separate chapter of MICAD (www.micad.nih.gov) (10).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=CCKR+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Mouse cholecystokinin B receptor (CCK2R (http://www.ncbi.nlm.nih.gov/gene/12426)); NCBI-Gene ID: 12426

Mouse CCK2R nucleotide and protein (http://www.genome.jp/dbget-bin/www_bget?mmu:12426) sequences in Kyoto Encyclopedia of Genes and Genomes database (KEGG)

KEGG pathway (Mouse CCK2R (http://www.genome.jp/dbget-bin/get_linkdb?-t+pathway+mmu:12426))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=cholecystokinin+receptor) related to cholecystokinin receptor

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20synthesis&cmd=DetailsSearch)]

The synthesis of [^111^In]-DOTA-sCCK8, [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H)], [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] has been described elsewhere (6). The radiochemical yields of the labeled peptides were not reported. The radiochemical purity of each labeled peptide was >95%, as determined with reversed-phase high-performance liquid chromatography (RP-HPLC) or instant thin-layer chromatography. The labeled peptides had a maximum specific activity of 5.5 GBq/μmol (203.5 mCi/μmol).

In another study, [^111^In]-DOTA-sCCK8, [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^111^In]-DOTA-MG0 were synthesized to investigate the biodistribution of these peptides in rodents bearing tumors (for details, see below) (9). These labeled peptides were reported to have a radiochemical purity of >95%; the radiochemical yield and specific activity of these tracers were not reported (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20in%20vitro%20studies&cmd=DetailsSearch)]

Using a phosphate-buffered saline/1-octanol mixture, the log P values (lipophilicity) of [^111^In]-DOTA-sCCK8, [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H)], [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] were determined to be −2.91 ± 0.20, −2.97 ± 0.02, −2.93 ± 0.13, and −2.86 ± 0.14, respectively (6). This indicated that the peptides were relatively hydrophobic and that the hydrophobicities of the different peptide derivatives were similar to that of the parent compound ([^111^In]-DOTA-sCCK8) (6).

The oxidation of [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Met^3,6^], [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] was investigated by incubating the peptides in a mixture of hydrogen peroxide, acetic acid, and ammonium acetate (in a ratio of 1:3:36) for 10 min at room temperature (6). RP-HPLC analysis of the peptides showed that ~66% of [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Met^3,6^] was oxidized, but the other two peptides showed no signs of oxidation.

The stability of the ^111^In-labeled peptides was studied by incubating the radiotracers in human serum for 4 h at 37°C (6). RP-HPLC analysis of the radiochemicals showed that, among all these peptides, only [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Met^3,6^] was slightly oxidized (2.3%).

Receptor binding and cellular internalization of the labeled peptides were investigated by incubating the different ^111^In-labeled tracers with HEK293 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1573&Template=cellBiology) cells (transfected with the CCK2R) for 2 h at 37°C (6). Results obtained from this study were presented as percent of total radioactivity added to the incubation mixture (Table 1).

Table 1: Receptor binding and cellular internalization of the ^ 111 ^ In-labeled sCCK8 peptide and its derivatives in CCK2R-transfected HEK293 cells ( 6 ).

Peptide | Percent of added radioactivity
Peptide | Bound to receptor | Internalized in cells
[^111^In]-DOTA-sCCK8 | 11.6 ± 0.7 | 35.2 ± 2.1
[^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H)] | 10.0–12.0 | ~13.0
[^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] | 10.0–12.0 | ~13.0
[^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] | 9.4 ± 0.6 | 26.8 ± 1.4

This study showed that the [^111^In]-DOTA-sCCK8 and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] had similar internalization kinetics, but the latter peptide showed ~7% lower internalization (P < 0.05) compared with the parent tracer (6).

Using a competitive binding assay with CCK2R-transfected HEK293 cells, the apparent IC_50_ values for DOTA-sCCK8, DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H)], DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] were determined to be 1.16 ± 0.06 nM, 27.2 ± 1.44 nM, 11.6 ± 1.06 nM, and 13.2 ± 1.12 nM, respectively (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-DOTA-sCCK8, [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H)], [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^] was investigated in athymic BALB/c nude mice bearing AR42J cell tumors (6). The animals (n = 5 mice/labeled peptide) were injected intravenously with 370 kBq (10 μCi; 0.1 μg) of the peptide, and the rodents were euthanized at 2 h postinjection (p.i.) to determine the amount of radioactivity that accumulated in the various tissues, including the tumors. For blocking studies, the animals (n = 5 mice/labeled peptide) were injected with the ^111^In-labeled peptide in the presence of 1,000-fold molar excess nonradioactive sCCK8. Results obtained from this study were presented as percentage of injected dose per gram tissue (% ID/g; Table 2).

Table 2: Uptake of radioactivity from different ^ 111 ^ In-labeled sCCK8 peptides in various tissues of athymic BALB/c nude mice bearing AR42J cell tumors ( 6 ).

[ ^ 111 ^ In]-DOTA peptide | Accumulated radioactivity (% of injected dose/gram tissue) | | | | | Tumor/blood ratio
[ ^ 111 ^ In]-DOTA peptide | Blood | Pancreas | Kidney | Stomach | Tumor | Tumor/blood ratio
sCCK8 | 0.03 ± 0.01 (0.02 ± 0.01)* | 2.01 ± 0.28 (0.24 ± 0.03) | 1.70 ± 0.17 (1.80 ± 0.16) | 0.69 ± 0.05 (0.17 ± 0.03) | 4.78 ± 0.64 (1.90 ± 0.16) | 189.64 ± 61.26 (91.12 ± 20.34)
sCCK8[Phe ^ 2 ^ (p-CH _ 2 _ SO _ 3 _ H)] | 0.02 ± 0.01 (0.02 ± 0.00) | 3.17 ± 0.74 (0.28 ± 0.03) | 1.40 ± 0.05 (1.58 ± 0.35) | 0.79 ± 0.06 (0.47 ± 0.19) | 2.18 ± 0.36 (0.58 ± 0.28) | 125.87 ± 51.68 (33.55 ± 16.00)
sCCK8[Phe ^ 2 ^ (p-CH _ 2 _ SO _ 3 _ H),HPG ^ 3,6 ^ ] | 0.04 ± 0.01 (0.06 ± 0.00) | 1.23 ± 0.14 (0.19 ± 0.16) | 1.48 ± 0.16 (2.03 ± 0.22) | 0.41 ± 0.05 (0.11 ± 0.04) | 1.92 ± 0.31 (0.44 ± 0.15) | 48.43 ± 12.01 (7.32 ± 2.91)
sCCK8[Phe ^ 2 ^ (p-CH _ 2 _ SO _ 3 _ H),Nle ^ 3,6 ^ ] | 0.03 ± 0.00 (0.03 ± 0.00) | 2.84 ± 0.19 (0.31 ± 0.08 | 1.35 ± 0.24 (1.53 ± 0.29) | 0.84 ± 0.14 (0.25 ± 0.02) | 4.54 ± 1.15 (1.40 ± 0.20) | 157.08 ± 35.42 (50.68 ± 5.97)

*Numbers in parenthesis represent uptake of radioactivity in animals given a blocking dose of sCCK8. For complete data, see Roosenburg et al. ( 6 ).

A significantly higher and similar uptake of radioactivity was observed in the tumors with [^111^In]-DOTA-sCCK8 (4.78 ± 0.64% ID/g) and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] (4.54 ± 1.15% ID/g) compared with the other tissues (P < 0.001) and peptides ([^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H)]: 2.18 ± 0.36% ID/g, P < 0.001; [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),HPG^3,6^]: 1.92 ± 0.31% ID/g, P < 0.001). In addition, accumulation of the tracer in the different tissues was blocked when an excess concentration of nonradioactive sCCK8 was co-injected with the radiolabeled peptides. This indicated that the uptake of label in the tumors and the other tissues was mediated through CCK2R. The pancreas, kidney, and stomach showed a higher uptake of radioactivity compared with the other organs (blood, lungs, muscle, spleen, and small intestines; each showed <0.5% ID/g accumulation of the label), and the investigators attributed this phenomenon to the presence of high concentrations of CCK2R in these organs (6). The tumor/blood ratios with [^111^In]-DOTA-sCCK8 and [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] were 189.64 ± 61.26 and 157.08 ± 35.42, respectively.

In another study, the biodistribution of [^111^In]-DOTA-sCCK8, [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], and [^111^In]-DOTA-MG0 was investigated in athymic BALB/c nude mice bearing tumors generated from A431 cells transfected with CCK2R (A431-CCK2R cells) (9). The animals (n = 5 mice/labeled peptide for each time point) were injected with 185 kBq (5 μCi, 0.03 nmol) of the ^111^In-labeled peptide, and the animals were euthanized 1 h p.i. and 4 h p.i. to determine the uptake of radioactivity in the various tissues, including the tumors (Table 3).

Table 3: Uptake of radioactivity from ^ 111 ^ In-labeled DOTA-sCCK8, DOTA-sCCK8[Phe ^ 2 ^ (p-CH _ 2 _ SO _ 3 _ H),Nle ^ 3,6 ^ ], and DOTA-MG0 peptides in A431-CCK2R cell tumors on athymic BALB/c nude mice ( 9 ).

[ ^ 111 ^ In]-DOTA-peptide | Uptake of radioactivity postinjection (% of injected dose/gram tissue)
[ ^ 111 ^ In]-DOTA-peptide | 1 h | 4 h
sCCK8 | 9.01 ± 1.75 | 5.74 ± 0.76
sCCK8[Phe ^ 2 ^ (p-CH _ 2 _ SO _ 3 _ H),Nle ^ 3,6 ^ ] | 4.95 ± 0.62 | 5.44 ± 0.41
MG0 | 12.5 ± 2.88 | ~10.0

For complete data, see Joosten et al. ( 9 ).

All three peptides targeted the tumors, but the uptake of radioactivity from [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] in the lesion was significantly lower (P < 0.01) than that with the other two peptides. However, with [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^], the uptake of label remained relatively constant from 1 h p.i. to 4 h p.i. The uptake of tracer in the kidneys was significantly higher with [^111^In]-DOTA-MG0 (70.3 ± 4.50% ID/g at 1 h p.i.) compared with either [^111^In]-DOTA-sCCK8 (1.46 ± 0.39% ID/g at 1 h p.i.; P < 0.01) or [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] (1.20 ± 0.10% ID/g at 1 h p.i.; P < 0.01). Coinjection of the labeled peptides with 1,000 molar excess nonradioactive peptide (n = 3 rodents/labeled peptide) reduced the uptake of radioactivity in the tumors by at least 50%, indicating that the ^111^In-labeled peptides had a high binding specificity for the CCK2R.

SPECT/computed tomography images of mice injected with the different ^111^In-labeled peptides were acquired at 1 h p.i. and 4 h p.i. as described by Joosten et al. (9). From the images it was evident that the tumor uptake of radioactivity with [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] was lower than that observed with the other two peptides. This observation was similar to the data obtained during the biodistribution study described above. With [^111^In]-DOTA-MG0, a very high uptake of label was observed in the kidneys.

From these studies, the investigators concluded that, because [^111^In]-DOTA-sCCK8[Phe^2^(p-CH_2_SO_3_H),Nle^3,6^] had a high in vivo stability, it is probably suitable for the noninvasive imaging and characterization of CCK2R in rodents (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-labeled%20CCK8%20peptide%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111in-labeled%20cck8%20peptide%20on%20human%20primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111in-labeled%20cck8%20peptide%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Laverman P., Sosabowski J.K., Boerman O.C., Oyen W.J. (2012). Radiolabelled peptides for oncological diagnosis. Eur J Nucl Med Mol Imaging.
2 Roosenburg S., Laverman P., van Delft F.L., Boerman O.C. (2011). Radiolabeled CCK/gastrin peptides for imaging and therapy of CCK2 receptor-expressing tumors. Amino Acids.
3 Laverman P., Roosenburg S., Gotthardt M., Park J., Oyen W.J., de Jong M., Hellmich M.R., Rutjes F.P., van Delft F.L., Boerman O.C. (2008). Targeting of a CCK(2) receptor splice variant with (111)In-labelled cholecystokinin-8 (CCK8) and (111)In-labelled minigastrin. Eur J Nucl Med Mol Imaging.
4 von Guggenberg E., Dietrich H., Skvortsova I., Gabriel M., Virgolini I.J., Decristoforo C. (2007). 99mTc-labelled HYNIC-minigastrin with reduced kidney uptake for targeting of CCK-2 receptor-positive tumours. Eur J Nucl Med Mol Imaging.
5 von Guggenberg E., Rangger C., Sosabowski J., Laverman P., Reubi J.C., Virgolini I.J., Decristoforo C. (2012). Preclinical Evaluation of Radiolabeled DOTA-Derivatized Cyclic Minigastrin Analogs for Targeting Cholecystokinin Receptor Expressing Malignancies. Mol Imaging Biol.
6 Roosenburg S., Laverman P., Joosten L., Eek A., Oyen W.J., de Jong M., Rutjes F.P., van Delft F.L., Boerman O.C. (2010). Stabilized (111)In-labeled sCCK8 analogues for targeting CCK2-receptor positive tumors: synthesis and evaluation. Bioconjug Chem.
7 von Guggenberg E., Sallegger W., Helbok A., Ocak M., King R., Mather S.J., Decristoforo C. (2009). Cyclic minigastrin analogues for gastrin receptor scintigraphy with technetium-99m: preclinical evaluation. J Med Chem.
8 Kosowicz J., Mikolajczak R., Czepczynski R., Ziemnicka K., Gryczynska M., Sowinski J. (2007). Two peptide receptor ligands (99m)Tc-EDDA/HYNIC-Tyr(3)-octreotide and (99m)Tc-EDDA/HYNIC-(D)Glu-octagastrin for scintigraphy of medullary thyroid carcinoma. Cancer Biother Radiopharm.
9 Joosten L., Laverman P., Boerman O.C., Roosenburg S., Eek A., Rutjes F.P., van Delft F.L. (2012). In vitro and in vivo characterization of three 68Ga- and 111 In-labeled peptides for cholecystokinin receptor imaging. Mol Imaging.
10 Chopra, A., 68Ga-Labeled DOTA conjugate of sCCK8[Phe2(p-CH2SO3H),Nle3,6], a sulfated cholecystokinin 8 (sCCK8) peptide derivative Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.